# Microbubbles conjugated with single-chain Cys-tagged vascular endothelial growth factor-121

Chemical name: | Microbubbles conjugated with single-chain Cys-tagged vascular endothelial growth factor-121
Abbreviated name: | scVEGF-MBs
Synonym:
Agent Category: | Polypeptide
Target: | Vascular endothelial growth factor receptor-2 (VEGFR-2)
Target Category: | Receptor
Method of detection: | Ultrasound
Source of signal / contrast: | Microbubbles (MBs)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB)]

Ultrasound is the most widely used imaging modality (1) and its role in noninvasive molecular imaging is expanding with ligand-carrying microbubbles (MBs) (2). MBs are composed of spherical cavities filled by a gas encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin, or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of MBs. MBs are usually 1–8 μm in diameter, and they provide a strongly reflective interface and resonate to ultrasound waves. MBs are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (3-5). They also have the potential to be used for drug and gene delivery (6).

Vascular endothelial growth factor (VEGF) consists of at least six isoforms with various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (7). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types, and they are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species (8). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFRs) on endothelial cells (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4). Several types of non-endothelial cells, such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells, also express VEGFRs (7).

VEGFRs have been found to be overexpressed in various tumor cells and tumor-associated endothelial cells but are not detectable in quiescent endothelial cells (9). Inhibition of VEGFR function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (10, 11). Radiolabeled VEGF has been developed as a tracer for imaging solid tumors and angiogenesis in humans (12-14). MBs conjugated to either peptides or antibodies against integrins, cell adhesion molecules, and VEGFRs have previously been studied for the non-invasive assessment and imaging of tumor angiogenesis (15-18). A 15-amino-acid long fusion tag (Cys-tag) was developed for site-specific conjugation via the free sulfhydryl group of Cys. Backer et al. (19) prepared a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF, which binds to VEGFR-2. In this chapter, Anderson et al. (20) studied ultrasonic imaging of tumor vasculature using MBs conjugated with scVEGF (scVEGF-MBs) in mice bearing human tumor xenografts.

### Related Resource Links:

- Chapters in MICAD (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=VEGFR+AND+micad%5Bbook%5D))
- Gene information in NCBI (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3791))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VEGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=VEGFR))
- Clinical trials (VEGFR (http://www.clinicaltrials.gov/ct2/results?term=VEGFR))
- FDA Drug information (VEGFR (http://google2.fda.gov/search?q=VEGFR&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB+synthesis)]

Backer et al. (19) reported the synthesis of a Cys-tagged vector of VEGF_121_ by cloning two single-chain 3–112 amino acid fragments of VEGF_121_ joining head-to-tail to express as scVEGF in Escherichia coli for mammalian cell production. Maleimide-bearing MBs (maleimide-MB) were reacted with a thio-containing scVEGF construct for 2 h at room temperature (20). scVEGF-MBs had a mean diameter of 2.5 ± 1.0 µm. There were 1.2 × 10^5^ scVEGF molecules per MB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB+in+vitro+studies)]

Anderson et al. (20) reported that scVEGF-MBs or maleimide-MBs (5 × 10^6^/ml) perfused for 5 min through flow chambers coated with VEGFR-2–positive porcine aortic endothelial cells at a wall shear rate of 1.0 dyne/cm^2^. There was a significantly (P < 0.01) greater number of scVEGF-MBs attached to the endothelial cells (25 ± 4 MBs/cell) than maleimide-MBs (5 ± 1 MBs/cell). In vitro ultrasound studies were performed using flow assay with agar phantom, which was immobilized with murine VEGFR-2 or control casein. The mean pixel amplitude of adherent scVEGF-MBs (1 × 10^6^/ml) was significantly higher (P < 0.01) in VEGFR-2–coated phantom (7 ± 2 dB) than in casein-coated phantom (0.2 dB).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB+rodentia)]

Anderson et al. (20) performed an ultrasound assessment of MB binding in mice bearing murine MC-38 colon adenocarcinoma tumors. Ultrasound was performed at 6 min after injection of scVEGF-MBs or maleimide-MBs (2 × 10^7^/mouse). The mean pixel amplitudes in the tumor were 8.46 ± 1.61 dB and 1.58 ± 0.83 dB for scVEGF-MBs and maleimide-MBs, respectively. The contrast enhancement of scVEGF-MBs to the tumors was significantly higher than that of maleimide-MBs (P < 0.01). The tumor contrast induced by scVEGF-MBs returned to background level (~1 dB) when a high M1, destructive acoustic pulse was administered to the tumor tissues. However, no blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=scVEGF%20MB%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=scVEGF%20MB+Human+Studies)]

No references are currently available.

## NIH Support

1R43 EB007857, 2R44 EB007857, 2R44 CA113080

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
5 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
6 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
7 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
8 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
9 Itakura J., Ishiwata T., Shen B., Kornmann M., Korc M. (2000). Concomitant over-expression of vascular endothelial growth factor and its receptors in pancreatic cancer. Int J Cancer.
10 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
11 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
12 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
13 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
14 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
15 Villanueva F.S., Jankowski R.J., Klibanov S., Pina M.L., Alber S.M., Watkins S.C., Brandenburger G.H., Wagner W.R. (1998). Microbubbles targeted to intercellular adhesion molecule-1 bind to activated coronary artery endothelial cells. Circulation.
16 Weller G.E., Lu E., Csikari M.M., Klibanov A.L., Fischer D., Wagner W.R., Villanueva F.S. (2003). Ultrasound imaging of acute cardiac transplant rejection with microbubbles targeted to intercellular adhesion molecule-1. Circulation.
17 Weller G.E., Villanueva F.S., Klibanov A.L., Wagner W.R. (2002). Modulating targeted adhesion of an ultrasound contrast agent to dysfunctional endothelium. Ann Biomed Eng.
18 Reinhardt M., Hauff P., Linker R.A., Briel A., Gold R., Rieckmann P., Becker G., Toyka K.V., Maurer M., Schirner M. (2005). Ultrasound derived imaging and quantification of cell adhesion molecules in experimental autoimmune encephalomyelitis (EAE) by Sensitive Particle Acoustic Quantification (SPAQ). Neuroimage.
19 Backer M.V., Patel V., Jehning B.T., Claffey K.P., Backer J.M. (2006). Surface immobilization of active vascular endothelial growth factor via a cysteine-containing tag. Biomaterials.
20 Anderson C.R., Rychak J.J., Backer M., Backer J., Ley K., Klibanov A.L. (2010). scVEGF microbubble ultrasound contrast agents: a novel probe for ultrasound molecular imaging of tumor angiogenesis. Invest Radiol.